# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-HER2-specific Affibody Z_HER2:2891_

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-synthetic HER2-specific Affibody Z_HER2:2891_
Abbreviated name: | ^68^Ga-DOTA-Z_HER2:2891_
Synonym: | ^68^Ga-ABY025
Agent category: | Affibody, antibody fragment
Target: | Epidermal growth factor receptor (EGFR, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891)]

Epidermal growth factor (EGF) is a 53-amino acid growth factor (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16); however, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed on the basis of a 58-amino acid (6.5 kDa) Z-domain residue from one of the IgG_1_-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <100 pM. Various radiolabeled Affibody molecules have been studied with regard to their utility for imaging HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. DOTA-Z_HER2:2891_, also known as ABY025, is a synthetic Affibody molecule that was produced for labeling with ^68^Ga. Kramer-Marek et al. (18) prepared ^68^Ga-DOTA-Z_HER2:2891_ for use with positron emission tomography (PET) imaging of HER2-positive tumors.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20synthesis)]

DOTA-Z_HER2:2891_ in ammonium acetate buffer (pH 4) was mixed with ^68^GaCl_3_. The mixture was incubated for 15 min at 80°C (18). ^68^Ga-DOTA-Z_HER2:2891_ was purified with column chromatography, with a radiochemical purity of >98%. Specific activity of ^68^Ga-DOTA-Z_HER2:2891_ was 2.8–5.2 GBq/nmol (76–141 mCi/nmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20in%20vitro)]

In vitro saturation binding assays of ^68^Ga-DOTA-Z_HER2:2891_ to human breast carcinoma MDA-MB-361 cells expressing HER2 receptor were performed (18). There was a single class of high-affinity binding sites, with a K_d_ value of 1.4 ± 0.9 nM and a B_max_ value of 9.7 ± 0.02 × 10^5^ HER2 receptors per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20rodentia)]

Kramer-Marek et al. (18) performed ex vivo biodistribution studies of 3.7–6.7 MBq (0.1–0.2 mCi) ^68^Ga-DOTA-Z_HER2:2891_ in nude mice (n = 4/group) bearing human breast carcinoma BT474 xenografts (high HER2 expression). There was a rapid clearance of ^68^Ga-DOTA-Z_HER2:2891_ from blood, with an elimination half-life of 20.8 min. ^68^Ga-DOTA-Z_HER2:2891_ remained >91% intact in the plasma at 2 h after injection. The tumor radioactivity was 31.0 ± 2.1% injected dose per gram (ID/g) at 1 h and 25.7 ± 2.2% ID/g at 3 h, and the tumor/blood ratios were 27 and 92, respectively. The radioactivity levels in the blood (0.28% ID/g), lung (0.56% ID/g), spleen (0.49% ID/g), bone (0.47% ID/g), pancreas (0.38% ID/g), and muscle (0.14% ID/g) were low at 3 h after injection. Radioactivity in the liver and gastrointestinal tract was <2% ID/g at 1 h and 3 h after injection, whereas the radioactivity in the kidneys was very high (>222% ID/g) at 1 h and 3 h after injection. Injection of a labeled control Affibody (^68^Ga-DOTA-His6-Z_Taq_) showed high kidney (172 ± 12.5% ID/g) and low tumor (1.1 ± 0.4% ID/g) accumulation at 1 h after injection. No blocking studies were performed.

PET imaging studies were performed in mice bearing BT474 tumors (high HER2 expression), MAD-MB-361 tumors (moderate HER2 expression) or MCF7 tumors (low HER2 expression) at 1 h after injection of 3.7–6.7 MBq (0.1–0.2 mCi) ^68^Ga-DOTA-Z_HER2:2891_ (18). The tumors and kidneys were clearly visualized. The radioactivity levels in the tumors were higher than in normal tissues, except in the kidneys. Region-of-interest analysis of tumors showed that the highest accumulation was in the BT474 tumors (31.0 ± 7.0% ID/g), followed by the MAD-MB-361 tumors (18.8 ± 2.5% ID/g) and MCF7 tumors (3.2 ± 0.4% ID/g). There was a significant correlation between % ID/g values obtained from ex vivo biodistribution and PET quantification studies (R^2^ = 0.94, P < 0.0001) in all tumor-bearing mice. Injection of ^68^Ga-DOTA-His6-Z_Taq_ in a mouse bearing a BT474 tumor showed little accumulation in the tumor at 1 h after injection. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=68Ga%20HER2%202891%20and%20human)]

No publication is currently available.

## NIH Support

Intramural research program

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Kramer-Marek G., Shenoy N., Seidel J., Griffiths G.L., Choyke P., Capala J. (2011). 68Ga-DOTA-affibody molecule for in vivo assessment of HER2/neu expression with PET. Eur J Nucl Med Mol Imaging.